# Cy5.5-Conjugated glycol chitosan-5β-cholanic acid nanoparticles

Chemical name: | Cy5.5-Conjugated glycol chitosan-5β-cholanic nanoparticles
Abbreviated name: | Cy5.5-CNPs
Synonym:
Agent Category: | Nanoparticles
Target: | Non-targeted
Target Category: | Non-targeted
Method of detection: | Optical imaging (near-infrared fluorescence (NIRF) imaging)
Source of signal / contrast: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=glycol%20chitosan%20nanoparticles&cmd=DetailsSearch)]

Researchers have developed and are in the process of evaluating a variety of nanoparticles (NPs) that can be structurally customized to deliver imaging agents or antineoplastic drugs for the detection and/or treatment of various cancers (1). The main advantage of using NPs to deliver an imaging probe or a therapeutic drug is that, compared to conventional delivery options, NPs can transport larger amounts of a payload, within the probe or on its surface, because they have a high surface area to volume ratio (1, 2). Although the size of the NPs determines its circulation time and the route of excretion from the body (NPs <10 nm in size are removed through the kidneys and those that are 10–200 nm are taken out of circulation by the reticuloendothelial system), the chemical composition of an NP affects its functions in vivo; for more information on NPs, see Jokerst and Gambhir (3) and Fox et al. (4). Small sized NPs that are cleared from blood circulation may pass through gaps of 2–6 nm that are present in the vascular endothelium and accumulate to some extent in healthy tissues, but they are eventually removed by the lymphatic system and returned into blood circulation. Compared to normal tissues, solid tumors show a much higher uptake and prolonged retention of the NPs (known as the enhanced permeation and retention effect (EPR); for details, see Reddy (5)) because the vasculature in these lesions is leaky due to the presence of large pores (up to 1 μm) (4). In addition, reduced blood flow through the neoplastic lesion and an impaired lymphatic system leads to very little removal of NPs accumulated in the tumor (4). However, in vivo studies have shown that some types of NPs may not have optimal biodistribution in the body and tend to accumulate in tumors because of their surface chemistry, charge, size, etc.

NPs made of glycol chitosan-5β-cholanic acid, a water-soluble, biocompatible, biodegradable, and self-aggregating carbohydrate polymer (CNPs), have been shown in different models to have good potential to target therapeutic drugs to tumors (6). Factors considered important for the use of NPs to carry and deliver imaging agents or drugs to tumors are stability (for extended circulation), deformability (to avoid unwanted penetration and accumulation in angiogenic blood vessels), and the ability to be taken up rapidly by tumor cells (6). For the CNPs, these parameters have been studied primarily in vitro, and no studies have been performed to investigate these characteristic of the particles under in vivo conditions (6). The CNPs were labeled with Cy5.5, a near-infrared (NIRF) dye, and the labeled NPs (Cy5.5-CNPs) were investigated for their stability, deformability, and rapid uptake in tumor cells and in mice bearing neoplastic lesions on the flank (established with human squamous cell carcinoma SCC7 cells), brain (established with glioblastoma U87 (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-14&Template=cellBiology) cells), liver (established with murine colon cancer CT26 (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2638&Template=cellBiology) cells), and metastatic tumors (established with RFP-B16F10 cells; mouse melanoma cells transfected with the red fluorescent protein (RFP) gene) (6).

### Related Resource Links

Nanoparticle-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books?term=%28nanoparticle%5BAll%20Fields%5D%20OR%20nanoparticles%5BAll%20Fields%5D%20OR%20nanotubes%5BAll%20Fields%5D%20OR%20%22iron%20oxide%22%5BAll%20Fields%5D%29%20AND%20micad%5Bbook%5D%20AND%20table%5Btype%5D&cmd=DetailsSearch)

Chitosan-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books?term=Chitosan%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D&cmd=DetailsSearch)

Fluorescent dye–related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books?term=%28Fluorescent%5BAll%20Fields%5D%20AND%20dye%5BAll%20Fields%5D%29%20AND%20micad%5Bbook%5D&cmd=DetailsSearch)

Optical imaging–related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books?term=Optical%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D%20AND%20table%5Btype%5D&cmd=DetailsSearch)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Cy5.5-CNPs%20synthesis&cmd=DetailsSearch)]

The synthesis of glycol chitosan-5β-cholanic acid and its labeling with Cy5.5 have been described by Na et al. (6). Each molecule of glycol chitosan was reported to have 150 ± 4.5 molecules of 5β-cholanic acid as determined with a colloidal titration method. Measurement of the extinction coefficient of Cy5.5 in the final preparation of Cy5.5-CNPs showed that there were 4.8 ± 0.7 molecules of Cy5.5 attached to each molecule of glycol chitosan-5β-cholanic acid. Dynamic light scattering analysis and transmission electron microscopy of CNPs dissolved in distilled water or in phosphate-buffered saline (pH 7.4) showed that they self-assembled into spherical NPs with an average diameter of 264 ± 30 nm (6).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Cy5.5-CNPs%20in%20vitro&cmd=DetailsSearch)]

It has been shown that, compared with 90% of the Cy5.5-conjugated CNPs that could pass through a 0.2-μm filter membrane, most of the smaller polystyrene NPs (PSs; diameter = 210 ± 10 nm) could not pass through the membrane (6). This indicated that the Cy5.5-NPs were partially deformable compared with the PSs. This phenomenon could be repeated even after the Cy5.5-NPs were incubated in a 0.15-μM solution of human serum albumin (HSA) for 1 day at 37°C. This indicated the Cy5.5-NPs were stable in HSA for at least 24 h at physiological temperature.

The uptake of PSs and Cy5.5-NPs by HUVEC (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1730&Template=cellBiology) cells (a human umbilical vein endothelial cell line), RAW264.7 (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=TIB-71&Template=cellBiology) cells (a murine macrophage cell line), and SCC7 cells, respectively, was compared by Na et al. (6). Fluorescence microscopy showed that all cell lines took up the PSs, and maximum accumulation of these particles was observed in the RAW264.7 cells. The higher uptake of the labeled NPs by the RAW264.7 cells was attributed to the phagocytic nature of these cells. A low uptake of Cy5.5-NPs was observed in the HUVEC and RAW264.7 cells, but the NPs showed a rapid and high accumulation in the cytosol of the SCC7 tumor cells (within 30 min after exposure), indicating that the NIRF dye conjugated particles probably have an ability to specifically target tumor cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Cy5.5-CNPs%20rodentia&cmd=DetailsSearch)]

To investigate the in vivo uptake of NPs by neoplastic tumor tissues, anesthetized athymic nude mice (n = 5 animals/group) bearing SCC7 cell lesions on the flank were injected with a solution of either Cy5.5-NPs (5 mg/kg body weight) or PSs (5 mg/kg body weight) through the tail vein (6). Subsequently, whole-body NIRF imaging was performed on the animals as described by Na et al. (6). At 1 h postinjection (p.i.), a strong fluorescence was observed throughout the body of the mice injected with the Cy5.5-NPs. By 1 day p.i., the tumors on the flank of these animals were clearly distinguishable from the surrounding normal tissue, indicating that the Cy5.5-NPs had the ability to specifically target the tumors in the rodents. A histological examination of the tumors and the normal surrounding tissues of the animals showed that the NPs were present only in the tumor sections. This observation confirmed the results obtained from the NIRF images described above. In addition, the photon count per gram of ex vivo tumor tissue was 35-fold higher than that of other organs, including the liver and the spleen. By comparison, the PSs accumulated primarily in the liver of the mice and had a very low NIRF signal in the tumor. The Cy5.5-Nps, compared with the PSs, were reported to have a much longer blood circulation time (6).

Real-time intravascular dynamic NIRF imaging of mice injected with the Cy5.5-NPs or the PSs (n = 5 experiments) showed that the two particle types behaved differently in the vascular tissues of the animals (6). The dye-conjugated NPs were observed to move rapidly through the vasculature, and by 5 min p.i. these particles were located primarily in the tumor blood vessels. Over time, the Cy5.5-NPs showed a high rate of diffusion and accumulation into the deeper parts of the lesion. This behavior was not apparent in the normal blood vessels (e.g., in the colon tissue) and showed that rapid permeation of the Cy5.5-NPs at the angiogenic sites such as those in a tumor was a characteristic feature of the labeled NPs. By comparison, most of the PSs were cleared from circulation and accumulated in the liver of the rodents.

The brain tumor targeting specificity of Cy5.5-NPs was evaluated in anesthetized mice (n = 5 animals) bearing U87 glioblastoma cell tumors in the organ and on the dorsal flank as described by Na et al. (6). Control animals were injected with saline in the brain and had no tumors on the flank. The rodents were injected with Cy5.5-NPs as before, and whole-body NIRF images were acquired at 1, 14, and 21 days p.i. Although the tumors on the flank were clearly visible at 1 day p.i., the brain tumor could not be distinguished from the surrounding tissue at this time point. At 14 days p.i., a clear NIRF signal was obtained from both the tumors in the test mice, and the intensity of the signal was reported to peak in both the tumors by 21 days p.i. No NIRF signal was visible in the control mice. This demonstrated that growth of the tumor resulted in partial breakdown of the blood–brain barrier, which allowed vasculature-specific penetration of the NPs into the brain lesions. These observations were confirmed with ex vivo NIRF imaging of the tumors obtained from the brain and the flank of the mice.

In a liver tumor model (n = 5 mice bearing CT26 cell tumors in the right lobe of the organ), the investigators showed that the Cy5.5-NPs accumulated specifically in the tumors and that the NIRF signal from the lesions increased from 1 h to 24 h p.i (6). Ex vivo NIRF imaging and histological examination of the liver showed that the fluorescence signal was intense only on the right side of the organ and not in the whole organ. This indicated that the labeled NPs could avoid the reticuloendothelial system and accumulated primarily in the tumor cells of the liver.

To distinguish metastatic tumor cells from normal cells, anesthetized nude mice (n = 5 animals) bearing RFP-B16F10 cell tumors were injected with the fluorescent CNPs as before (6). Whole-body NIRF imaging of the animals showed that the fluorescence signal was generated only from the lung region of the mice. Analysis of the fluorescence signal with z-stack imaging (http://www.zeiss.de/C12567BE0045ACF1/Contents-Frame/6A9B2F1F9EC90DFAC1256E300033C4F8) showed that the labeled NPs were localized and spread in the whole organ. Ex vivo analysis of the lungs showed there was a high expression of the RFP in the organ, and NIRF imaging showed accumulation of the Cy5.5-NPs in the lungs, thus confirming the presence of metastatic cancer in the tissue.

From these studies, the investigators concluded that Cy5.5-CNPs have a high stability and deformability and could be taken up rapidly by tumor cells in rodents (6).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Cy5.5-CNPs%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Cy5.5-CNPs%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Cy5.5-CNPs%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Banerjee D., Sengupta S. (2011). Nanoparticles in cancer chemotherapy. Prog Mol Biol Transl Sci.
2 Kim B.Y., Rutka J.T., Chan W.C. (2010). Nanomedicine. N Engl J Med.
3 Jokerst J.V., Gambhir S.S. (2011). Molecular imaging with theranostic nanoparticles. Acc Chem Res.
4 Fox M.E., Szoka F.C., Frechet J.M. (2009). Soluble polymer carriers for the treatment of cancer: the importance of molecular architecture. Acc Chem Res.
5 Reddy L.H. (2005). Drug delivery to tumours: recent strategies. J Pharm Pharmacol.
6 Na J.H., Koo H., Lee S., Min K.H., Park K., Yoo H., Lee S.H., Park J.H., Kwon I.C., Jeong S.Y., Kim K. (2011). Real-time and non-invasive optical imaging of tumor-targeting glycol chitosan nanoparticles in various tumor models. Biomaterials.